# Trastuzumab-dextran iron oxide nanoparticles

Chemical name: | Trastuzumab-dextran iron oxide nanoparticles
Abbreviated name: | Trastuzumab-dextran NP
Synonym: | Herceptin-dextran NP
Agent Category: | Humanized monoclonal antibody
Target: | HER2 or ErbB2/neu receptor
Target Category: | Antibody-receptor binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of Signal/Contrast: | Iron oxide nanoparticles
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the human nucleotide and protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=194688152) sequence of HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=herceptin+dextran)]

Breast cancer tumors that express high levels of human epidermal growth factor receptor 2 (commonly known as HER2/neu or the ErbB-2 receptor; also designated as the cluster of differentiation 340 (CD340)) indicate a poor prognosis for the patient because this receptor promotes rapid proliferation and spread of cancer cells into the surrounding tissues (1-3). Trastuzumab, a humanized monoclonal antibody (MAb) against HER2/neu, is commercially available in the United States. This MAb is approved (http://www.fda.gov/cder/foi/label/2008/103792s5175lbl.pdf) by the United States Food and Drug Administration for the treatment of the primary and metastatic forms of breast cancer. This MAb is also being evaluated in clinical trials (http://clinicaltrials.gov/ct2/results?term=Herceptin) for the treatment of a variety of cancers. Because of its specificity for tumors expressing the HER2/neu receptor, trastuzumab has been conjugated with a variety of radionuclides and used for the diagnosis of various cancer types, including breast cancer, using different imaging techniques (4, 5).

Investigators have recently developed a series of new contrast agents that contain superparamagnetic iron oxide (SPIO) particles that can be used to visualize different tissue pathologies, including cancers, with magnetic resonance imaging (MRI) (6, 7). The particles have also been used in several in vivo applications such as immunoassays, disease diagnosis, drug delivery, and biological fluid detoxification (8-11). To make the SPIO particles biocompatible with the mammalian system, the particles are chemically cross-linked with polymers such as dextran, polyethylene glycols, and polyvinylpyrrolidines that have themselves been used as drug carriers. Chen et al. used dextran cross-linked iron oxide nanoparticles (CLIO NPs) to conjugate trastuzumab and used the trastuzumab-NPs for the in vitro detection of HER2/neu expression in breast cancer cell lines (12). The NPs were also used for the in vivo MRI imaging of mice bearing breast cancer tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=dextran+herceptin)]

The synthesis of trastuzumab-dextran iron oxide NP was described by Chen et al. (12). Briefly, the SPIO particles were prepared by mixing dextran-T40 with an aqueous solution of ferric and ferrous chloride at room temperature followed by the addition of ammonium hydroxide. The mixture was stirred for 1 hr and centrifuged to remove any aggregated particles. The SPIO NPs were then purified from excess dextran with gel filtration chromatography on a Sephacryl S-300 column. The dextran-coated SPIO NPs were reported to elute in the void volume under these chromatographic conditions. Iron concentration of the SPIO NPs was determined as described by Chen et al. (12). The cross-linking of dextran on the SPIO NPs to obtain the CLIO NP was achieved by stirring the dextran-coated SPIO NPs with a solution of epichlorohydrin and sodium hydroxide for 24 h at room temperature. The CLIO NPs were subsequently purified with dialysis against several changes of distilled water. The CLIO NPs were then incubated with 2,2’-(ethylenedioxy)bisethylamine (EDBE) for 24 h at room temperature to generate the primary amine groups at the end of dextran and to obtain the CLIO-EDBE NPs. Purification of the CLIO-EDBE NPs was achieved with dialysis against distilled water as described above. Generation of the various NPs (SPIO, CLIO, and CLIO-EDBE) was confirmed with Fourier transform infrared spectroscopy.

To generate the trastuzumab-NPs, the CLIO-EDBE NPs were incubated with commercially available trastuzumab in a solution containing 1-hydroxybenzotriazole and (benzotriazole-1-yloxy)tripyrrolidinophosphonium hexafluorophosphate at room temperature for 24 h (12). Unbound trastuzumab was removed with gel filtration chromatography on a Sephadex-G25 column, and the trastuzumab-NPs were eluted in phosphate-buffered saline (PBS) (the pH of PBS used for the elution was not mentioned in the publication).

The core size of the trastuzumab-NPs was 3.5 ± 0.3 nm as determined with transmission electron microscopy (12). The number of trastuzumab molecules/NP was not reported in the publication (12). The pH-dependent stability of trastuzumab-NP was investigated by dispersing the NPs in PBS (pH 7.4) and in buffers with pH values ranging from 4 to 10 (12). The NPs were reported to show no aggregation at any pH for at least 4 months as confirmed with the dynamic light-scattering technique. The investigators also reported that the r_1_ and r_2_ relaxivity values, as measured at 20 MHz with a relaxometer, showed little change over 4 months at 37.0 ± 0.1°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=dextran+and+herceptin)]

Human breast cancer cell lines SKBR3, BT-474, MDA-MB-231, and MCF-7 that express HER2/neu receptors were used to study the in vitro cytotoxicity and receptor targeting of trastuzumab-NP (12). For this study the KB human nasopharyngeal epidermal carcinoma cell line, which does not express HER2/neu receptors, was used as a control. For the cytotoxicity study an equal number of cells of the respective cell lines were exposed to trastuzumab-NP at concentrations ranging from 1 to 10 mM Fe. It was reported although trastuzumab-NP was not cytotoxic to any cell line at the lowest concentration (1 mM Fe), it was observed to be toxic to all cell lines at higher concentrations (5 and 10 mM Fe) (12). The receptor targeting of trastuzumab-NP was studied with the same cell lines mentioned above using a concentration of 1 mM Fe (12). After exposure to trastuzumab-NP, the cells were treated with an anti-human IgG (γ-chain) conjugated to fluorescein isothiocyanate (anti-human IgG-FITC). The cells were washed with PBS and fixed with paraformaldehyde for observation under a confocal microscope. Only cells expressing the HER2/neu receptors (BT-474, SKBR-3, MDA-MB-231, and MCF-7) were reported to show fluorescence (MDA-MB-231> BT-474> SKBR-3≥ MCF-7) with the anti-human IgG-FITC conjugate, indicating that the trastuzumab-NPs specifically bound to the HER2/neu receptors on these cells.

In another study the different cell lines were respectively exposed to trastuzumab-NP (0.3 mM Fe), washed with PBS, and scanned with a magnetic resonance scanner (12). As expected, only cells expressing the HER2/neu receptor were reported to show a negative enhancement of the MRI signal. No such negative enhancement was evident with the control KB cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=dextran+herceptin+rodentia)]

Nude mice (n = 5) bearing SKBR-3 (HER2/neu expressing) and KB (HER2/neu non-expressing) cell tumors in the left and right lateral thighs, respectively, were used to investigate the targeting of HER2/neu expressing and non-expressing tumors by trastuzumab-NP (12). The T_2_-weighted fast spin-echo imaging was performed on the mice 1 h after an intravenous injection of trastuzumab-NP. Compared with the signal with the KB cell tumors, a significant drop in the T_2_-weighted signal was reported only with the SKBR-3 cell tumors (P values were not reported). This indicated that the trastuzumab-NPs specifically targeted the tumors expressing HER2/neu. No competition study using trastuzumab-NP after a pre-treatment of the animals with trastuzumab alone was reported.

The biodistribution of trastuzumab-NP was investigated in 18 male ICR (http://www.informatics.jax.org/external/festing/mouse/docs/ICR.shtml) mice after an intravenous injection (20 μmol/kg) of the NPs (12). The animals were euthanized at various time intervals up to 24 h after injection, and the blood, brain, heart, lungs, liver, spleen, and the kidneys from the mice were harvested. The respective organs were washed with PBS, and the Fe concentration of each whole organ was measured with inductively coupled plasma mass spectrometry. The results were reported as a percentage of injected dose per gram of tissue (% ID/g). The serum Fe concentration was reported to increase for 1 h after injection, and it remained stable up to 1.5 h. Subsequently, at 24 h the serum Fe concentration was reported to drop to background levels. The brain showed almost no accumulation of the NPs. The heart showed an increase in Fe concentration up to 30 min after injection, and the increase in concentration remained fairly stable up to 24 h. The lungs showed an increase in accumulation of the NPs from 15 to 30 min, and subsequently the concentration was reduced by 24 h after the injection. Compared to the other organs, the liver and kidneys showed a lower and fairly stable accumulation of the NPs up to 24 h after treatment. The spleen showed an increased NP accumulation, reaching a maximum of ~600% ID/g; however, this organ had a high background Fe level (~300% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=herceptin+dextran+non+primate+mammals)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=herceptin+dextran+non+human+primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=herceptin+dextran+human+studies)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

Boxes can have a single level of sections; the titles for these sections should be marked up in “Box subhead” style.

## References

1 Milanezi F., Carvalho S., Schmitt F.C. (2008). EGFR/HER2 in breast cancer: a biological approach for molecular diagnosis and therapy. Expert Rev Mol Diagn.
2 Pupa S.M., Tagliabue E., Menard S., Anichini A. (2005). HER-2: a biomarker at the crossroads of breast cancer immunotherapy and molecular medicine. J Cell Physiol.
3 Azim H., Azim H.A. (2008). Targeting Her-2/neu in breast cancer: as easy as this!. Oncology.
4 Stipsanelli E., Valsamaki P. (2005). Monoclonal antibodies: old and new trends in breast cancer imaging and therapeutic approach. Hell J Nucl Med.
5 Koyama Y., Hama Y., Urano Y., Nguyen D.M., Choyke P.L., Kobayashi H. (2007). Spectral fluorescence molecular imaging of lung metastases targeting HER2/neu. Clin Cancer Res.
6 Kiessling, F., Noninvasive cell tracking. Handb Exp Pharmacol, 2008(185 Pt 2): p. 305-21.
7 Margolis D.J., Hoffman J.M., Herfkens R.J., Jeffrey R.B., Quon A., Gambhir S.S. (2007). Molecular imaging techniques in body imaging. Radiology.
8 Schellenberger E., Schnorr J., Reutelingsperger C., Ungethum L., Meyer W., Taupitz M., Hamm B. (2008). Linking proteins with anionic nanoparticles via protamine: ultrasmall protein-coupled probes for magnetic resonance imaging of apoptosis. Small.
9 Sun C., Veiseh O., Gunn J., Fang C., Hansen S., Lee D., Sze R., Ellenbogen R.G., Olson J., Zhang M. (2008). In vivo MRI detection of gliomas by chlorotoxin-conjugated superparamagnetic nanoprobes. Small.
10 Kalambur V.S., Longmire E.K., Bischof J.C. (2007). Cellular level loading and heating of superparamagnetic iron oxide nanoparticles. Langmuir.
11 Caputo A., Sparnacci K., Ensoli B., Tondelli L. (2008). Functional polymeric nano/microparticles for surface adsorption and delivery of protein and DNA vaccines. Curr Drug Deliv.
12 Chen, T.J., T.H. Cheng, C.Y. Chen, S.C. Hsu, T.L. Cheng, G.C. Liu, and Y.M. Wang, Targeted Herceptin-dextran iron oxide nanoparticles for noninvasive imaging of HER2/neu receptors using MRI. J Biol Inorg Chem, 2008